# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-triacetic acid-human serum albumin-Ac-Cys-Z_EGFR:1907_

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-triacetic acid-human serum albumin-Ac-Cys-Z_EGFR:1907_
Abbreviated name: | ^64^Cu-DO3A-HSA-Z_EGFR:1907_
Synonym:
Agent category: | Antibody, Affibody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Positron emission tomography
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells, such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use in anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2, based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A, was constructed (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. The EGFR-specific Affibody Z_EGFR:1907_ (6.7 kDa) was identified to have good affinity (K_d_ = 5.4 nM) for EGFR (HER1) and labeled with ^111^In via isothiocyanate-benzoyl-diethylenetriamine pentaacetic acid (DTPA) to form ^111^In-Bz-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/) for single-photon emission computed tomography (18) imaging in nude mice bearing human tumors (19). To facilitate site-specific conjugation, Ac-Cys-Z_EGFR:1907_ (Cys at the N terminal) was synthesized and conjugated with 1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidethylacetamide (maleimido-mono-amide-DOTA) to form Ac-Cys(DOTA)-Z_EGFR:1907_ (DOTA-Z_EGFR:1907_), and the product was labeled with ^64^Cu (t_1/2_, 12.7 h) to form ^64^Cu-DOTA-Z_EGFR:1907_ for positron emission tomography (20) imaging studies in tumor-bearing mice (21). Although high specific tumor accumulation was observed with ^111^In- and ^64^Cu-labeled Z_EGFR:1907_, very high kidney accumulation (>100% injected dose per gram (ID/g)) was also observed. Addition of human serum albumin (HSA) to Affibody Z_HER2:342_ dramatically reduced kidney accumulation and improved tumor accumulation (22). Therefore, Hoppmann et al. (23) prepared ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7-triacetic acid-human serum albumin-Z_EGFR:1907_ (^64^Cu-DO3A-HSA-Z_EGFR:1907_) for evaluation showing good PET tumor contrast with low kidney accumulation in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR+1907+synthesis)]

Ac-Cys-Z_EGFR:1907_ was prepared with automated solid-phase peptide synthesizer (23). DOTA-N-hydroxysuccinimide ester and HSA (100:1 molar ratio) were incubated in borate buffer (pH 8.5) for 2 h at 4°C to form DO3A-HSA, which was isolated with PD-10 column chromatography. DO3A-HSA was then reacted with sulfosuccinimidyl 4-[N-maleimidomethyl]cyclohexane-1-carboxylate (Sulfo-SMCC) in a molar ratio of 1:5 for 1 h at 4°C. The resulting bioconjugate was further purified with PD-10 column chromatography. Ac-Cys-Z_EGFR:1907_ was conjugated in a site-specific manner to the DOTA and Sulfo-SMCC modified HSA via the cysteine residue. The reaction was performed in a molar ratio of 1:5 of DO3A-HSA-SMCC and Ac-Cys-Z_EGFR:1907_ (22 nmol) for 6 h at room temperature. DO3A-HSA-Z_EGFR:1907_ was purified with ultracentrifugation. There were an average of three DO3A moieties and two Ac-Cys-Z_EGFR:1907_ moieties per HSA protein as determined with MALDI-TOF-MS and sodium dodecyl sulfate polyacrylamide gel electrophoresis (SDS-PAGE). Approximately 2.4 nmol DO3A-HSA-Z_EGFR:1907_ was radiolabeled with ^64^Cu by addition of 37 MBq (1 mCi) ^64^CuCl_2_ in 0.1 N sodium acetate buffer (pH 6.0) and incubated for 1 h at 39°C. ^64^Cu-DO3A-HSA-Z_EGFR:1907_ was isolated with PD-10 column chromatography, with >70% radiolabeling yield. ^64^Cu-DO3A-HSA-Z_EGFR:1907_ exhibited a specific activity of ~14 MBq/nmol (0.38 mCi/nmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20in%20vitro)]

^64^Cu-DO3A-HSA-Z_EGFR:1907_ accumulated in SAS human oral squamous carcinoma cells with 26.8 ± 2.5% incubation dose at 37°C for 2 h (23). Co-incubation with excess Ac-Cys-Z_EGFR:1907_ reduced the accumulation to 9.6 ± 1.5% incubation dose. The K_d_ value of ^64^Cu-DO3A-HSA-Z_EGFR:1907_ for EGFR of SAS cells was not determined.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20rodentia)]

PET static imaging analysis was performed in nude mice (n = 4) bearing SAS tumors at 1, 4, 24, 48, and 72 h after intravenous injection of 6.7–7.8 MBq (0.18–0.21 mCi) ^64^Cu-DO3A-HSA-Z_EGFR:1907_ (~0.5 nmol) (23). The tumor was clearly visualized at 24–72 h. Quantification analysis showed that the tumor accumulation levels were 3.3 ± 0.2% ID/g, 5.2 ± 0.4% ID/g, 7.0 ± 1.1% ID/g, 7.7 ± 1.1% ID/g, and 7.5 ± 1.0% ID/g at 1, 4, 24, 48, and 72 h, respectively. At 24 h, the liver and kidney accumulation levels were 11.3 ± 1.1% ID/g and 2.5 ± 1.7% ID/g, respectively. The kidney accumulation (2.5% ID/g) of ^64^Cu-DO3A-HSA-Z_EGFR:1907_ was drastically reduced compared with ^64^Cu-DOTA -Z_EGFR:1907_ (88.4% ID/g) (21). At 1–72 h, the blood levels were <5% ID/g, and the muscle levels were <2% ID/g. No blocking and ex vivo biodistribution studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20human)]

No publication is currently available.

## NIH Support

5R01 CA119053, P50 CA114747

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Goldman E.R., O'Shaughnessy T.J., Soto C.M., Patterson C.H., Taitt C.R., Spector M.S., Charles P.T. (2004). Detection of proteins cross-linked within galactoside polyacrylate-based hydrogels by means of a quantum dot fluororeagent. Anal Bioanal Chem.
19 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
20 Gao X., Yang L., Petros J.A., Marshall F.F., Simons J.W., Nie S. (2005). In vivo molecular and cellular imaging with quantum dots. Curr Opin Biotechnol.
21 Miao Z., Ren G., Liu H., Jiang L., Cheng Z. (2010). Small-animal PET imaging of human epidermal growth factor receptor positive tumor with a 64Cu labeled affibody protein. Bioconjug Chem.
22 Hoppmann S., Miao Z., Liu S., Liu H., Ren G., Bao A., Cheng Z. (2011). Radiolabeled affibody-albumin bioconjugates for HER2-positive cancer targeting. Bioconjug Chem.
23 Hoppmann S., Qi S., Miao Z., Liu H., Jiang H., Cutler C.S., Bao A., Cheng Z. (2012). (177)Lu-DO3A-HSA-Z (EGFR:1907): characterization as a potential radiopharmaceutical for radionuclide therapy of EGFR-expressing head and neck carcinomas. J Biol Inorg Chem.